# Copper pyruvaldehyde bis(N^4^-methylthiosemicarbazone) complex

Chemical name: | Copper pyruvaldehyde bis(N^4^-methylthiosemicarbazone) complex
Abbreviated name : | Cu-PTSM, Cu(PTSM)
Synonym:
Agent Category: | Compound
Target: | Cu
Target Category: | Redox trapping mechanism, reduction of Cu(II) to Cu(I)
Method of detection: | PET
Source of signal : | ^62^Cu
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%20pyruvaldehyde%20bis%28N%284%29-methylthiosemicarbazone%29%20complex%22%5BSubstance%20Name%5D)]

Copper pyruvaldehyde bis(N^4^-methylthiosemicarbazone) complex, or Cu-PTSM, is a positron emission tomography (PET) radiopharmaceutical that can be used to evaluate blood flow in the heart, brain, and tumors (1, 2). Cu-PTSM belongs to a class of neutral, lipophilic complexes that have demonstrated rapid diffusion into cells. Animal studies have also demonstrated its therapeutic potential to inhibit cancer cell implantation and growth at doses that resulted in no overt signs of toxicity (3).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%20pyruvaldehyde%20bis%28N%284%29-methylthiosemicarbazone%29%20complex%22%5BSubstance%20Name%5D%20AND%20%22synthesis%22%5BAll%20Fields%5D)]

Cu-PTSM can be synthesized using the method described by Petering et al. (4). Nevertheless, it can be obtained more efficiently using a ^62^Zn/^62^Cu PET generator [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%20pyruvaldehyde%20bis%28N%284%29-methylthiosemicarbazone%29%20complex%22%5BSubstance%20Name%5D%20AND%20%22generator-produced%22%5BText%20Word%5D)]. One system described by Mathias et al. (5) integrates the generator into a device for the preparation and purification of the radiopharmaceutical. This system enables the synthesis of ^62^Cu-PTSM in <8 min with a radiochemical yield of about 40% and a purity of >98%. Zweit et al. (6) developed and optimized a high-activity ^62^Zn/^62^Cu PET generator, enabling direct labeling of Cu-PTSM with a 94% radiochemical yield. One system described by Haynes et al. (7) uses purified ^62^Zn loaded onto a generator column in 2 M HCl, which is then eluted using an internal three-channel peristaltic pump. The pump delivers 2.25 ml of eluant (1.8 M NaCl, 0.2 M HCl) through the generator column to elute the ^62^Cu in 40 s.

As reported by Fujibayashi et al. (8), ^62^Cu can be easily eluted as a neutral ^62^Cu-glycine solution, and PTSM labeling can be complemented by mixing the ^62^Cu-eluate with a PTSM solution. This simple elution/labeling procedure, coupled with the short half-life of ^62^Cu, allows clinical studies to be repeated easily (9).

Experimental determinations of dose calibrator settings for generator-produced ^62^Cu-PTSM were performed by Zimmerman and Cessna (10) using a measurement model developed at National Institute of Standards and Technology (NIST) for short-lived radionuclides.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%20pyruvaldehyde%20bis%28N%284%29-methylthiosemicarbazone%29%20complex%22%5BSubstance%20Name%5D%20AND%20%22in%20vitro%22%5BAll%20Fields%5D)]

Several in vitro studies have demonstrated the potential therapeutic value of ^64^Cu-PTSM in various forms of cancer. Using a hamster model of colorectal cancer that mimics the implantation of cancer cells after invasive surgery (11), Lewis et al. (12) showed a rapid uptake of Cu-PTSM in single-cell suspensions, thus demonstrating an inhibition of cancer cell implantation and growth at doses well below the maximum tolerated dose, with no signs of toxicity to the animals.

Electron spin resonance (ESR) spectrometry studies and high-performance liquid chromatography (HPLC) analysis of ^62^Cu-PTSM in tumor cell lines showed that, in the brain, a mitochondrial electron transport enzyme reduced Cu-PTSM specifically, but Cu-PTSM was not reduced in tumor mitochondria. The reduction was enzymatic and NADH dependent, possibly similar to the activation mechanism of bioreductive anticancer drugs (8, 13). In murine brain homogenate, ESR and HPLC analysis indicated the reduction and cleavage of Cu(II)-PTSM to Cu(I). This virtually irreversible reduction was specifically initiated by the mitochondrial enzymatic system.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%20pyruvaldehyde%20bis%28N%284%29-methylthiosemicarbazone%29%20complex%22%5BSubstance%20Name%5D%20AND%20%22rodentia%22%5BMeSH%5D)]

In rat model systems, Cu-PTSM showed excellent uptake in the brain and heart after intravenous injection, exhibiting a microsphere-like retention in the brain and heart (14, 15). Cu-PTSM was shown to be an effective cell radiolabeling agent in ex vivo/in vivo PET studies of cell trafficking in mice, with a labeling procedure of minimal cytotoxicity. Adonai et al. (16) showed maximum cytotoxicity of Cu-PTSM after 180 min, with a labeling efficiency directly proportional to ^64^Cu-PTSM concentration and influenced negatively by serum. In comparison with FDG, uptake of ^64^Cu-PTSM was more efficient (3) .

Studies performed on hamsters with colorectal carcinoma cell implants (GW39) showed that ^64,67^Cu-PTSM could be used to quantify tumor blood flow (17). Because of the relationship between the trapping mechanism of Cu-PTSM (which is thought to result from a reductive decomposition of the copper(II) complex by intracellular sulfhydryls) and glutathione levels in the tissue, and because tumor tissue glutathione levels might vary, the temporal uptake of Cu-PTSM was investigated by PET in both tumor-bearing hamsters and rats bearing R3227 prostate tumors. Results showed that the tumors were clearly visualized, and the retained copper radioactivity in the tumor was constant over the 30-min imaging period. Similarly, Barnhart-Bott and Green (18) investigated the possible effects of glutathione depletion on the biodistribution of ^67^Cu-PTSM in rats and showed that only very small changes in the biodistribution of copper-labeled Cu-PTSM occurred in the treated rats compared with untreated controls.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%20pyruvaldehyde%20bis%28N%284%29-methylthiosemicarbazone%29%20complex%22%5BSubstance%20Name%5D%20AND%20%28dogs%20OR%20rabbits%20OR%20birds%29)]

Studies on dogs with spontaneously occurring soft-tissue neoplasms were performed to evaluate whether [^62^Cu]Cu-PTSM could serve as a blood flow tracer in PET studies of tumor tissue (19). Results indicate that an excellent linear correlation exists between tumor perfusion calculated from [^62^Cu]Cu-PTSM data and tumor perfusion measured with ^85^Sr-microspheres (r = 0.94 for 80 samples), suggesting that [^62^Cu]Cu-PTSM might be useful as a radiopharmaceutical for PET studies of tumor perfusion. Ultrafiltration and plasma/erythrocyte partitioning studies to assess the protein binding of ^67^Cu-labeled Cu-PTSM revealed significant interspecies variability in the strength of Cu-PTSM binding to serum albumin, with ^67^Cu-PTSM binding much more strongly to human albumin than to dog albumin (20).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%20pyruvaldehyde%20bis%28N%284%29-methylthiosemicarbazone%29%20complex%22%5BSubstance%20Name%5D%20AND%20%28%22Primates%22%5BMeSH%5D%20NOT%20%22humans%22%5BMeSH%5D%25)]

Very few investigations using primate models are reported in the literature. A study by Mathias et al. (21) using baboon single-pass cerebral extraction measurements confirmed the potential of generator-produced ^62^Cu-PTSM for cerebral perfusion PET imaging. Experiments were carried out with the use of ^67^Cu (t_1/2_ = 2.6 days), ^64^Cu (t_1/2_ = 12.7 h), and ^62^Cu (t_1/2_ = 9.7 min), respectively. All three chelates were extracted into the brain with high efficiency and showed some clearance in the 10-50-second time frame.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper%20pyruvaldehyde%20bis%28N%284%29-methylthiosemicarbazone%29%20complex%22%5BSubstance%20Name%5D%20AND%20%22Human%22%5BAll%20Fields%5D)]

^62^Cu-PTSM PET was shown to be an effective means of detecting occlusive coronary artery disease in humans and to quantify cerebral and myocardial blood flow [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22copper%20pyruvaldehyde%20bis%28N%284%29-methylthiosemicarbazone%29%20complex%22%5BSubstance%20Name%5D%20OR%20Cu-PTSM%5BText%20Word%5D%29%20AND%20coronary%5BAll%20Fiel)]. In the study by Wallhaus et al. (22), ^62^Cu-PTSM myocardial perfusion defects were identified in 100% of patients with three-vessel disease (n = 8), 100% of patients with two-vessel disease (n = 9), and 67% of patients with single-vessel disease (n = 6). In the case of individual vessels, ^62^Cu-PTSM perfusion defects were seen in 72% of patients with occlusive disease in the left anterior descending artery territory, 67% in the left circumflex artery territory, and 60% in the right coronary artery territory, respectively.

Nevertheless, despite promising results in animals, ^62^Cu-PTSM myocardial uptake using PET was found to be greatly reduced in humans because of the binding of the tracer to human serum albumin (HSA) (20, 23, 24). A way to counteract the binding to HSA is to add a free acid (e.g., stearic acid). In their study on the release of Cu-PTSM from HSA by fatty acids, Yuan et al. (23) showed that Cu-PTSM was completely released from HSA when the ratio of spin-labeled stearic acid to HSA was 5:1.

^62^Cu-PTSM appears to be a clinically safe radiopharmaceutical with favorable dosimetry for human studies at injected doses significantly above those projected for use in clinical studies. Human biodistribution studies performed by Wallhaus et al. (25) showed the liver to be the critical organ for radiation absorbed dose estimates (0.0886 rad/mCi), defining the maximum single injected dose at 56 mCi, using the limit of 5 rads to a critical organ per study per year. The whole-body dose was 0.0111 rad/mCi, resulting in a 0.622-rad exposure with a maximum single injection dose. Only trace levels of activity were found in the urine, suggesting low levels of urinary excretion and bladder exposure. No significant clinical, electrocardiographic, or laboratory abnormalities were seen after the injection of ^62^Cu-PTSM.

Quantitative studies of tracer uptake for investigating angiotensin II-induced changes in blood flow distribution in the liver showed that ^62^Cu-PTSM-PET was a valuable blood flow assessment method for patients receiving angiotensin II infusions (26).

## References

1 Herrero P, et al. (1996). Regional myocardial perfusion assessed with generator-produced copper-62-PTSM and PET. J Nucl Med.
2 Taniuchi H, et al. (1997). Hyperfixation of copper-62-PTSM in rat brain after transient global ischemia. J Nucl Med.
3 Lewis JS, et al. (2002). Copper-64-pyruvaldehyde-bis(N(4)-methylthiosemicarbazone) for the prevention of tumor growth at wound sites following laparoscopic surgery: monitoring therapy response with microPET and magnetic resonance imaging. Cancer Res.
4 Petering HG, Buskirk HH, Underwood GE. (1964). The Anti-Tumor Activity Of 2-Keto-3-Ethoxybutyraldehyde Bis(Thiosemicarbazone) And Related Compounds. Cancer Res.
5 Mathias CJ, et al. (1991). A remote system for the synthesis of copper-62 labeled Cu(PTSM). Int J Rad Appl Instrum [A].
6 Zweit J, et al. (1992). Development of a high performance zinc-62/copper-62 radionuclide generator for positron emission tomography. Eur J Nucl Med.
7 Haynes NG, et al. (2000). Performance of a 62Zn/62Cu generator in clinical trials of PET perfusion agent 62Cu-PTSM. J Nucl Med.
8 Fujibayashi Y, et al. (1993). Mitochondria-selective reduction of 62Cu-pyruvaldehyde bis(N4-methylthiosemicarbazone) (62Cu-PTSM) in the murine brain; a novel radiopharmaceutical for brain positron emission tomography (PET) imaging. Biol Pharm Bull.
9 Matsumoto K, et al. (1992). Application of the new zinc-62/copper-62 generator: an effective labeling method for 62Cu-PTSM. Int J Rad Appl Instrum B.
10 Zimmerman BE, Cessna JT. (1999). The standardization of 62Cu and experimental determinations of dose calibrator settings for generator-produced 62CuPTSM. Appl Radiat Isot.
11 Wu JS, et al. (1997). Implantation of colon cancer at trocar sites is increased by low pressure pneumoperitoneum. Surgery.
12 Lewis JS, et al. (1999). Evaluation of 64Cu-ATSM in vitro and in vivo in a hypoxic tumor model. J Nucl Med.
13 Shibuya K, et al. (1999). Cytosolic/microsomal redox pathway: a reductive retention mechanism of a PET-oncology tracer, cu-pyruvaldehyde-bis(N4-methylthiosemicarbazone) (cu-PTSM). Ann Nucl Med.
14 Green MA. (1987). A potential copper radiopharmaceutical for imaging the heart and brain: copper-labeled pyruvaldehyde bis(N4-methylthiosemicarbazone). Int J Rad Appl Instrum B.
15 Green MA, Klippenstein DL, Tennison JR. (1988). Copper(II) bis(thiosemicarbazone) complexes as potential tracers for evaluation of cerebral and myocardial blood flow with PET. J Nucl Med.
16 Adonai N, et al. (2002). Ex vivo cell labeling with 64Cu-pyruvaldehyde-bis(N4-methylthiosemicarbazone) for imaging cell trafficking in mice with positron-emission tomography. Proc Natl Acad Sci U S A.
17 Mathias CJ, et al. (1991). Investigation of copper-PTSM as a PET tracer for tumor blood flow. Int J Rad Appl Instrum B.
18 Barnhart-Bott A, Green MA. (1991). The effects of glutathione depletion on the biodistribution of Cu(PTSM) in rats. Int J Rad Appl Instrum B.
19 Mathias CJ, et al. (1994). Evaluation of Cu-PTSM as a tracer of tumor perfusion: comparison with labeled microspheres in spontaneous canine neoplasms. Nucl Med Biol.
20 Mathias CJ, Bergmann SR, Green MA. (1995). Species-dependent binding of copper(II) bis(thiosemicarbazone) radiopharmaceuticals to serum albumin. J Nucl Med.
21 Mathias CJ, et al. (1990). Evaluation of a potential generator-produced PET tracer for cerebral perfusion imaging: single-pass cerebral extraction measurements and imaging with radiolabeled Cu-PTSM. J Nucl Med.
22 Wallhaus TR, et al. (2001). Copper-62-pyruvaldehyde bis(N-methyl-thiosemicarbazone) PET imaging in the detection of coronary artery disease in humans. J Nucl Cardiol.
23 Yuan H, et al. (1996). Release of CuPTSM from human serum albumin after addition of fatty acids. J Inorg Biochem.
24 Mathias CJ, et al. (1991). In vivo comparison of copper blood-pool agents: potential radiopharmaceuticals for use with copper-62. J Nucl Med.
25 Wallhaus TR, et al. (1998). Human biodistribution and dosimetry of the PET perfusion agent copper-62-PTSM. J Nucl Med.
26 Flower MA, et al. (2001). 62Cu-PTSM and PET used for the assessment of angiotensin II-induced blood flow changes in patients with colorectal liver metastases. Eur J Nucl Med.